# ^99m^Tc-Hydrazinonicotinamide-anti-TAG-72 CC49 divalent single-chain Fv monoclonal antibody

Chemical name: | ^99m^Tc-Hydrazinonicotinamide-anti-TAG-72 CC49 divalent single-chain Fv monoclonal antibody
Abbreviated name: | ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb
Synonym: | ^99m^Tc-CC49 sc(Fv)_2_ MAb, ^99m^Tc-CC49 MAb
Agent Category: | Divalent single-chain Fv monoclonal antibody (sc(Fv)_2_ MAb
Target: | TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal/ contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

^99m^Tc-Hydrazinonicotinamide-anti-TAG-72 CC49 divalent single-chain Fv monoclonal antibody (^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb), which is formed by the conjugation of ^99m^Tc with a bioengineered anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for single-photon emission computed tomography (SPECT) imaging of cancers that express TAG-72 (1). ^99m^Tc is a gamma emitter with a half-life (t_½_) of 6.02 h.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (2-5). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (6). The murine MAb B72.3 against TAG-72 was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (7). With use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-2 MAbs with higher affinity constants (K_a_) have been produced and characterized (1-3, 7).

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (8). Radiolabeled B72.3 and CC49 have shown excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (9, 10). Because of their relatively large size, radiolabeled intact MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (1, 11-13). One approach to minimize these problems is reducing intact antibodies to antibody fragments such as F(ab’)_2_ and Fab’ (14). Another approach is the development of genetic engineering methods to obtain single-chain Fv constructs (scFv) and multivalent scFv constructs (1, 15, 16). These scFv constructs contain the variable regions of the light chain (V_L_) and heavy chain (V_H_) connected by a flexible linker. Colcher et al. (17) constructed the monomeric CC49 scFv MAb (~27 kDa), which selectively recognizes a unique sialyl-Tn epitope of TAG-72. The radioiodinated CC49 scFv appeared to clear rapidly from the blood with good tumor penetration (16, 18). To further improve the imaging kinetics, Pavlinkova et al. (18) constructed the high-affinity dimer CC49 sc(Fv)_2_ (~60 kDa). The radioiodinated CC49 sc(Fv)_2_ showed good stability and increased avidity in vivo compared with the radioiodinated CC49 scFv construct.

With direct or indirect labeling, MAbs can be labeled with ^99m^Tc, a gamma emitter with ideal SPECT imaging properties. Direct labeling involves reduction of ^99m^Tc-pertechnetate and nonspecific binding of the reduced ^99m^Tc to donor atoms, namely thiol, amide, amino, and carboxylate (19). Indirect labeling uses a bifunctional chelating agent, which can be more binding site–specific on the MAb molecule. Goel et al. (1) used hydrazinonicotinamide (HYNIC) as a bifunctional coupling agent to label CC49 sc(Fv)_2_ with ^99m^Tc. The ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb showed good tumor targeting and in vivo biodistribution properties.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

Goel et al. (1) reported the construction and radiolabeling of the ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb. The CC49 scFv (V_L_-linker-V_H_) was derived from the murine MAb CC49 cloned in the yeast expression vector pPICZαA and constructed with the 205C linker. The bacterial scFv construct was used as the template DNA for the expression of the scFv in competent P. pastoris KM71 cells. The construction of the divalent sc(Fv)_2_ (V_L_-linker-V_H_-linker-V_L_-linker-V_H_-His_6_) was performed as described by Goel et al. (20) using the 205C linker in a P. pastoris expression system, and the final construct was purified from the secreted medium with immobilized metal affinity chromatography. The preparation was shown to be >95% pure by sodium dodecylsulfate-polyacrylamide gel electrophoresis (SDS-PAGE). Size-exclusion high-performance liquid chromatography (HPLC) showed the molecular mass to be 60 kDa. Competitive solid-phase competition enzyme-linked immunosorbent assay (ELISA) with bovine submaxillary gland mucin (BSM) confirmed the immunoreactivity of the divalent construct. To radiolabel the agent, the hydrazino-modification of CC49 sc(Fv)_2_ was achieved by reacting the construct with the N-hydroxysuccinimide ester of succinimidyl-6-hydrazinonicotinate hydrochloride (SHNH) at a molar ratio of 10:1 in sodium phosphate buffer (pH 7.8). It was estimated that there were ~2.3 SHNH groups per sc(Fv)_2_. In the radiolabeling procedure, sodium ^99m^Tc-pertechnetate, tricine, and stannous chloride were first mixed, then SHNH-derivatized CC49 sc(Fv)_2_ was added, and the reaction mixture was incubated at room temperature for 45 min. The final ^99m^Tc-HYNIC-CC49 sc(FV)_2_ MAb was purified on a Sephadex G-25 column. The specific activity was 74–111 MBq/mg (2–3 mCi/mg) or 4.44–6.66 MBq/nmol (0.12–0.18 mCi/nmol) on the basis of the estimated 60-kDa molecular weight) with a radiochemical purity ≥95% (HPLC analysis). On SDS-PAGE, >90% of the total radioactivity was associated with the protein band of 58 kDa.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

The immunoreactivity of ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb by solid-phase ELISA with immobilized BSM was 85–95% with a nonspecific binding of 0.8–1.5% (1).

In vitro stability studies of ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb were conducted by incubating the radiolabeled MAb construct in 1% bovine serum albumin (BSA) or 1% mouse serum at 37ºC for 24 h (1). By HPLC analysis, <20% loss of ^99m^Tc label was detected in 1% BSA. In the 1% mouse serum, ~20% and 10% of the ^99m^Tc were associated with low molecular weight proteins (<50 kDa) and high molecular weight proteins (>130 kDa), respectively. This latter protein fraction suggested the possibility of aggregation of the radiolabel with serum proteins.

Using the Scatchard plot and surface plasmon resonance technique to measure the real-time interactions, Goel et al. (21) reported the K_a_ of unlabeled CC49 sc(Fv)_2_ to be 2.75 × 10^7^ M−^1^ in binding to the immobilized BSM. In comparison, the K_a_ for the intact CC49 MAb construct was 1.14 × 10^8^ M−^1^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Biodistribution studies of ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb were performed in nude mice bearing LS-147T s.c. human colon carcinomas (~250–300 mm^3^) (1). Each mouse received 0.37 MBq (10 μCi) of ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ mAb by i.v. administration. The blood elimination t_½_ was 144 min, and the whole-body clearance t_½_ was 184 ± 19 min (n = 3). The radioactivity levels (n = 3 × 2) in percentage injected dose per gram (% ID/g) of the tumors were 9.9 ± 0.7 (0.5 h), 10.9 ± 0.8 (1 h), 12.6 ± 0.4 (4 h), 7.2 ± 0.7 (8 h), 2.3 ± 0.1 (16 h), and 1.2 ± 0.0 (24 h). At 16 h, the tumor/blood ratio was 4.6:1. At 0.5 h, the radioactivity levels (% ID/g) of major organs were 13.9 ± 1.1 (blood), 18.9 ± 1.5 (liver), 13.4 ± 1.2 (spleen), 33.9 ± 1.8 (kidneys), and 5.4 ± 0.8 (lungs). At 4 h, these levels changed to 4.3 ± 0.2 (blood), 14.8 ± 1.3 (liver), 9.7 ± 0.7 (spleen), 27.3 ± 1.4 (kidneys), and 1.3 ± 0.0 (lungs). By 24 h, these levels declined to 0.1 ± 0.0 (blood), 1.2 ± 0.0 (liver), 1.0 ± 0.0 (spleen), 2.4 ± 0.3 (kidneys), and 0.0 ± 0.0 (lungs). Macroautoradiography studies performed in mice at 6 h and 16 h after radioactivity administration confirmed a high degree of tumor localization and negligible retention in the blood and normal organs (1). The exceptions were the liver and pancreas, but the tumor radioactivity levels were still two-fold higher at both 6 and 16 h in these two organs. The tumor remained positive at 16 h after injection. The study suggested that ^99m^Tc-HYNIC-CC49 sc(Fv)_2_ MAb probably underwent hepatobiliary excretion.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No publication is currently available.

## References

1 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
2 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
3 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
4 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
5 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
6 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
7 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
8 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
9 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
10 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
11 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
12 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
13 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
14 Behr T. Becker W. Hannappel E. Goldenberg D.M. Wolf F. Targeting of liver metastases of colorectal cancer with IgG, F(ab')2, and Fab' anti-carcinoembryonic antigen antibodies labeled with 99mTc: the role of metabolism and kinetics Cancer Res 1995 55Suppl23 5777s 5785s 7493346
15 Bird R.E., Hardman K.D., Jacobson J.W., Johnson S., Kaufman B.M., Lee S.M., Lee T., Pope S.H., Riordan G.S., Whitlow M. (1988). Single-chain antigen-binding proteins. Science.
16 Colcher D., Bird R., Roselli M., Hardman K.D., Johnson S., Pope S., Dodd S.W., Pantoliano M.W., Milenic D.E., Schlom J. (1990). In vivo tumor targeting of a recombinant single-chain antigen-binding protein. J Natl Cancer Inst.
17 Colcher D., Goel A., Pavlinkova G., Beresford G., Booth B., Batra S.K. (1999). Effects of genetic engineering on the pharmacokinetics of antibodies. Q J Nucl Med.
18 Pavlinkova G., Beresford G.W., Booth B.J., Batra S.K., Colcher D. (1999). Pharmacokinetics and biodistribution of engineered single-chain antibody constructs of MAb CC49 in colon carcinoma xenografts. J Nucl Med.
19 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
20 Goel A., Beresford G.W., Colcher D., Pavlinkova G., Booth B.J., Baranowska-Kortylewicz J., Batra S.K. (2000). Divalent forms of CC49 single-chain antibody constructs in Pichia pastoris: expression, purification, and characterization. J Biochem (Tokyo).
21 Goel A., Colcher D., Baranowska-Kortylewicz J., Augustine S., Booth B.J., Pavlinkova G., Batra S.K. (2000). Genetically engineered tetravalent single-chain Fv of the pancarcinoma monoclonal antibody CC49: improved biodistribution and potential for therapeutic application. Cancer Res.